# [N-methyl-^11^C]4-(4-(4-Chlorophenyl)-4-hydroxypiperidin-1-yl)-2,2-diphenyl-N-methyl-butanamide

Chemical name: | [N-methyl-^11^C]4-(4-(4-Chlorophenyl)-4-hydroxypiperidin-1-yl)-2,2-diphenyl-N-methyl-butanamide
Abbreviated name: | [^11^C]dLop
Synonym: | [N-methyl-^11^C]N-desmethyl-loperamide
Agent category: | Compound
Target: | P-glycoprotein (Pgp), multidrug transporter
Target category: | Transporter
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide)]

One of the mechanisms of tumor cells to escape the cytotoxic effects of chemotherapeutic agents, such as adriamycin, vinca alkaloids, epipodophyllotoxins, actinomycin D, and paclitaxel, is to limit their presence inside the cells by a multidrug resistance (MDR-1) gene protein (1, 2). The MDR-1 gene encodes a transmembrane P-glycoprotein (P-gp) as an ATP-dependent multidrug transporter that is capable of actively pumping a variety of agents out of the cells. Injection of unlabeled efflux pump substrates increases the retention of the radioactivity in the tumor rather than less radioactivity as seen with receptor binding radiotracers. Over-expression of P-gp in tumor cells (such as renal carcinoma, hepatoma, pheochromocytoma, and colon carcinoma) leads to resistance to anticancer drugs (3). P-gp is also present in a variety of normal cells, such as intestinal mucosal cells, hepatocytes, renal proximal tubule epithelial cells, and endothelial cells of the blood brain barrier (BBB) (4, 5). Calcium channel blockers, cyclosporin and its non-immunosuppressive analogue PSC 833 are MDR modulators inhibiting transport of P-gp substrates out of the cells (6, 7).

Sestamibi (MIBI) is a substrate for P-gp. ^99m^Tc-MIBI has been approved by the FDA as a myocardial perfusion imaging agent with single photon emission computed tomography (SPECT) to assess the risk of future cardiac events (8). It is also used as a tumor-imaging agent in breast, lung, thyroid, and brain cancers (9-13). Loperamide is an opiate agonist (14) and an avid substrate for P-gp at the BBB (15). [^11^C]Loperamide ([^11^C]Lop) has been studied as a positron emission tomography (PET) agent for studying P-gp function and multidrug resistance in tumors and normal tissues non-invasively (16). However, demethylation of [^11^C]Lop to [N-methyl-^11^C]N-desmethyl-loperamide ([^11^C]dLop) precludes quantification of P-gp function with PET if [^11^C]dLop is also an avid substrate for P-gp. Therefore, [^11^C]dLop has been studied as a positron emission tomography (PET) agent for studying P-gp function and multidrug resistance in tumors and normal tissues non-invasively (17).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20synthesis)]

[^11^C]dLop was synthesized by a reaction of 4-(4-(4-chlorophenyl)-4-hydroxypiperidin-1-yl)-2,2-diphenylbutanamide with [^11^C]methyl iodide at 80°C for 6 min (17). The radiochemical purity of purified [^11^C]dLop was >99% with specific activities of 152 ± 48 GBq/µmol (4.11 ± 1.30 Ci/µmol) at the end of synthesis. The total synthesis time was 40 min with a radiochemical yield of 18% (decay-corrected) based on [^11^C]CO_2_.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20in%20vitro)]

In vitro binding studies using cloned receptors with dLop showed inhibition constant (K_i_) values were 0.56, 73 and 328 nM for µ, δ and κ opiate receptor, respectively (16). The measured Log D_7.4_ of [^11^C]dLop was 2.60.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20rodentia)]

PET imaging studies with [^11^C]dLop PET imaging in three normal and three P-gp knockout mice showed a higher accumulation of radioactivity in the forebrain in the knockout mice than the wide type mice by 3.6 fold (17). The maximal brain accumulation in the knockout mice occurred at 8-20 min after injection. Three hydrophilic radiometabolites were detected in the plasma and brains with high-performance liquid chromatography (HPLC). In the knockout mice, the fraction of unchanged [^11^C]dLop in the plasma and brain determined with HPLC was 7.7% and 92% at 60 min after injection, respectively. In the wide type mice, the fraction of unchanged [^11^C]dLop in the plasma and brain was 11.1% and 42.6% at 60 min after injection, respectively. The ex vivo brain concentrations of [^11^C]dLop were ~16-fold greater in the knockout mice than in wild-type mice, whereas little differences were observed in the plasma of these mice. There was a 7-fold increase in total ([^11^C]dLop plus its radiometabolites) radioactivity in the forebrain in the knockout mice as compared with the wide type mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20%28nonhuman%20primate%29)]

Lazarova et al. (17) showed that DCPQ (P-gp blocker, 8 mg/kg) pretreatment of six rhesus monkeys enhanced brain [^11^C]dLop PET radioactivity by 7-fold in the frontal cortex and 13-fold in the cerebellum at 30 min after injection. The increase of brain radioactivity was not blocked by administration of naloxone (opiate antagonist) or dLop at 30 min after [^11^C]dLop injection in the DCPQ-pretreated monkeys. Three hydrophilic radiometabolites were detected in monkey arterial plasma at as early as 10 min after injection. The fraction of unchanged [^11^C]dLop in the plasma was ~30% at 60 min after injection. DCPQ had little effect on the rate at which each radiometabolite appeared in the plasma. Liow et al. (18) performed similar PET studies showing that the brain (2% ID), liver (39% ID), lung (31% ID) and kidney (11% ID) were the main organs with visually accumulation of radioactivity at 2-30 min after injection. P-gp blockade increased the brain radioactivity to 3% ID, whereas no effects on the other organs. Furthermore, the accumulation of radioactivity among brain regions with P-gp blockade correlated linearly with blood flow, suggesting a high single-pass extraction.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C+Loperamide%20and%20%28%20human%29)]

Seneca et al. (19) performed whole-body scans for 120 min after injection of 744 MBq (20 mCi) [^11^C]dLop in 8 healthy subjects. The highest absorbed doses were in the kidneys (50.1 ± 6.0 µSv/MBq), spleen (30.5 ± 6.8 µSv/MBq), lungs (27.0 ± 3.4 µSv/MBq), thyroid (14.7 ± 6.2 µSv/MBq), liver (12.9 ± 2.7 µSv/MBq), and urinary bladder wall (10.8 ± 3.3 µSv/MBq). The effective dose (ED) was 7.6 ± 0.6 µSv/MBq. There were minimal brain uptake of [^11^C]dLop with the rate of brain entry of <0.01 mL.cm^-3^.min^-1^. The plasma concentration of [^11^C]dLop declined rapidly with a biexponential function. The half-lives were 0.4 and 15 min. The fraction of intact [^11^C]dLop in plasma was 85% at 5 and 120 min after injection. There were 5 hydrophilic radiometabolites.

## NIH Support

Intramural research program

## References

1 Endicott J.A., Ling V. (1989). The biochemistry of P-glycoprotein-mediated multidrug resistance. Annu Rev Biochem.
2 Gottesman M.M., Pastan I. (1993). Biochemistry of multidrug resistance mediated by the multidrug transporter. Annu Rev Biochem.
3 Fojo A.T., Ueda K., Slamon D.J., Poplack D.G., Gottesman M.M., Pastan I. (1987). Expression of a multidrug-resistance gene in human tumors and tissues. Proc Natl Acad Sci U S A.
4 Piwnica-Worms D., Rao V.V., Kronauge J.F., Croop J.M. (1995). Characterization of multidrug resistance P-glycoprotein transport function with an organotechnetium cation. Biochemistry.
5 Thiebaut F., Tsuruo T., Hamada H., Gottesman M.M., Pastan I., Willingham M.C. (1987). Cellular localization of the multidrug-resistance gene product P-glycoprotein in normal human tissues. Proc Natl Acad Sci U S A.
6 Hughes C.S., Vaden S.L., Manaugh C.A., Price G.S., Hudson L.C. (1998). Modulation of doxorubicin concentration by cyclosporin A in brain and testicular barrier tissues expressing P-glycoprotein in rats. J Neurooncol.
7 Mayer U., Wagenaar E., Dorobek B., Beijnen J.H., Borst P., Schinkel A.H. (1997). Full blockade of intestinal P-glycoprotein and extensive inhibition of blood-brain barrier P-glycoprotein by oral treatment of mice with PSC833. J Clin Invest.
8 Piwnica-Worms D., Chiu M.L., Budding M., Kronauge J.F., Kramer R.A., Croop J.M. (1993). Functional imaging of multidrug-resistant P-glycoprotein with an organotechnetium complex. Cancer Res.
9 Berman D.S., Kiat H., Van Train K., Garcia E., Friedman J., Maddahi J. (1991). Technetium 99m sestamibi in the assessment of chronic coronary artery disease. Semin Nucl Med.
10 George E.F., Komisar A., Scharf S.C., Ferracci A., Blaugrund S. (1998). Diagnostic value of the preoperative sestamibi scan in intraoperative localization of parathyroid adenomas: a case study. Laryngoscope.
11 Mansoor M.R., Heller G.V. (1997). Recent developments in the prognostic use of myocardial perfusion imaging. Curr Opin Cardiol.
12 Maublant J. (1997). Scintigraphic imaging of breast tumors. Eur J Radiol.
13 Vermeersch H., Loose D., Ham H., Otte A., Van de Wiele C. (2003). Nuclear medicine imaging for the assessment of primary and recurrent head and neck carcinoma using routinely available tracers. Eur J Nucl Med Mol Imaging.
14 Awouters F., Megens A., Verlinden M., Schuurkes J., Niemegeers C., Janssen P.A. (1993). Loperamide. Survey of studies on mechanism of its antidiarrheal activity. Dig Dis Sci.
15 Sadeque A.J., Wandel C., He H., Shah S., Wood A.J. (2000). Increased drug delivery to the brain by P-glycoprotein inhibition. Clin Pharmacol Ther.
16 Zoghbi S.S., Liow J.S., Yasuno F., Hong J., Tuan E., Lazarova N., Gladding R.L., Pike V.W., Innis R.B. (2008). 11C-loperamide and its N-desmethyl radiometabolite are avid substrates for brain permeability-glycoprotein efflux. J Nucl Med.
17 Lazarova N., Zoghbi S.S., Hong J., Seneca N., Tuan E., Gladding R.L., Liow J.S., Taku A., Innis R.B., Pike V.W. (2008). Synthesis and evaluation of [N-methyl-11C]N-desmethyl-loperamide as a new and improved PET radiotracer for imaging P-gp function. J Med Chem.
18 Liow J.S., Kreisl W., Zoghbi S.S., Lazarova N., Seneca N., Gladding R.L., Taku A., Herscovitch P., Pike V.W., Innis R.B. (2009). P-glycoprotein function at the blood-brain barrier imaged using 11C-N-desmethyl-loperamide in monkeys. J Nucl Med.
19 Seneca N., Zoghbi S.S., Liow J.S., Kreisl W., Herscovitch P., Jenko K., Gladding R.L., Taku A., Pike V.W., Innis R.B. (2009). Human Brain Imaging and Radiation Dosimetry of 11C-N-Desmethyl-Loperamide, a PET Radiotracer to Measure the Function of P-Glycoprotein. J Nucl Med.